# 3'-Deoxy-3'-[^18^F]fluorothymidine

Chemical name: | 3'-Deoxy-3'-[^18^F]fluorothymidine
Abbreviated name: | [^18^F]FLT, FLT
Synonym: | [^18^F]Fluorothymidine
Agent category: | Compound
Target: | Thymidine kinase-1
Target category: | Transporters, enzymes
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Humans | Structure is currently not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%5BAll%20Fields%5D%20AND%20fluorothymidine%5BAll%20Fields%5D%29%20OR%2018F-FLT)]

One of the characteristics of tumor cells is their unchecked proliferation. It is important to measure the proliferation rate of cancer lesions to help differentiate benign from malignant tumors and to characterize malignant tumors among normal tissues. 2-[^18^F]Fluoro-2-deoxy-D-glucose ([^18^F]FDG) has been widely used in cancer imaging. However, enhanced uptakes of FDG also occur in inflammatory cells and lesions as well as in necrotic cells (1, 2). Thymidine (TdR) and TdR analogs are the standard markers for DNA synthesis, and [^11^C]thymidine has been used in positron emission tomography (PET) imaging to measure tumor growth rate in situ. Because of the short half-life of ^11^C and extensive metabolism of [^11^C]TdR in the blood (3), 3'-deoxy-3'-[^18^F]fluorothymidine (FLT) was developed for PET imaging.

FLT is an analog of TdR and is phosphorylated by thymidine kinase-1 (TK-1), an enzyme expressed during the DNA synthesis phase of the cell cycle (4). Most cancer cells have a much higher TK-1 activity than normal cells. FLT monophosphate is not incorporated into DNA and is impermeable to the cell membrane. Therefore, it is metabolically trapped inside the cells. The uptake and accumulation of FLT are used as an index of cellular proliferation. [^18^F]FLT PET has been used to detect and monitor tumor proliferation, to evaluate the stages of tumor, and to detect metastases (5).

### Related Resource Links:

- Chapters in MICAD (Thymidine kinase (http://www.ncbi.nlm.nih.gov/books/?term=thymidine+kinase+AND+micad%5Bbook%5D))
- Gene information in NCBI (Thymidine kinase (http://www.ncbi.nlm.nih.gov/gene/7083))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Thymidine kinase (http://www.ncbi.nlm.nih.gov/omim/188300))
- Clinical trials ([^18^F]FLT (http://www.clinicaltrials.gov/ct2/results?term=FLT&Search=Search))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F-FLT%5BText%20Word%5D%20OR%20fluorothymidine%5BAll%20Fields%5D%29%20AND%20%28radiosynthesis%5BText%5D%20OR%20automated%5BAll%20Fields%5D%29)]

A reliable radiosynthesis of [^18^F]FLT has been developed based on [^18^F]fluoride displacement of a protected nosylate precursor. A simple three-step synthesis was used to prepare 370 MBq (>10 mCi) of radiochemically pure [^18^F]FLT, with a specific activity of 37 GBq/μmol (>1 Ci/μmol) at the end of synthesis within 100 min and with 13% radiochemical yield (end of bombardment; 7% end of synthesis) (6). Recently, Oh et al. (7) reported a new, fully automated method for the synthesis of [^18^F]FLT with a yield of 50% radiochemical yield, by modifying a commercial FDG synthesizer and its disposable fluid pathway.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%5BAll%20Fields%5D%20AND%20fluorothymidine%5BAll%20Fields%5D%29%20OR%20%28%22alovudine%22%5BSubstance%20Name%5D%20OR%2018F-FLT%5BText%20Word%5D%29%20AND%20in%20vitro)]

Expression of major pyrimidine metabolizing enzymes in pancreatic cancer cell lines, chronic pancreatitis tissue, and human pancreatic cancer and the in vitro uptake of [^18^F]FLT were studied (8). TK-1 and thymidine synthetase mRNA were increased in six pancreatic cancer cell lines. High TK-1 activity was confirmed in all of these cancer cell lines as compared with normal pancreatic tissue and samples from patients with chronic pancreatitis. The cellular uptake of [^18^F]FLT was 18.4% ± 3.6% and 5.2% ± 1.4% of the applied radioactivity after 240 min in SW-979 and BxPc-3 cells, respectively, whereas uptake of [^18^F]FDG was only 0.6% ± 0.04% (SW-979) and 0.3% ± 0.13% (BxPc-3). In contrast, the cellular uptake of [^18^F]FLT in isolated pancreas and growth-arrested HT1080 cells was lower as compared with the uptake of [^18^F]FDG and with the malignant pancreatic cancer cell lines. The majority of [^18^F]FLT was phosphorylated to the respective monophosphate in both cell lines. The incorporation of [^18^F]FLT into the DNA was only 0.8% ± 0.12% (BxPc-3) and 1.3% ± 0.38% (SW-979) of the applied radioactivity. These results demonstrate the cellular uptake, intracellular trapping, and incorporation into the DNA of [^18^F]FLT in pancreatic cancer cells in vitro. TK-1, as the rate-limiting enzyme of [^18^F]FLT metabolism, is overexpressed in pancreatic cancer cell lines and in human pancreatic cancer.

It was recently reported that human lung adenocarcinoma A549 cells accumulated [^18^F]FLT intracellularly as [^18^F]FLT-nucleotides (49% monophosphate, 6% diphosphate, and 29% triphosphate) by high-performance liquid chromatography (HPLC) analyses (9). The rate-limiting step in the overall conversion of FLT to FLT-triphosphate was the phosphorylation of the monophosphate by thymidylate kinase. FLT-triphosphate was resistant to degradation and trapped in the cells, although it was not incorporated into DNA.

Cells derived from human esophageal carcinoma were grown for 2 days and incubated with cisplatin, 5-fluorouracil (5-FU), methotrexate, or gemcitabine. The cytotoxic drugs methotrexate, 5-FU, and gemcitabine caused an increase in [^18^F]FLT accumulation with similar [^18^F]FDG uptake as compared with untreated cells. There was a rebound effect of the cancer cells to increase the uptake of FLT. The cytostatic drug, cisplatin, showed a decrease in [^18^F]FLT uptake and little change in [^18^F]FDG uptake (10). Not all of the anticancer drugs have the same effect on FLT uptake, depending on their mechanisms of action.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%20AND%20fluorothymidine%29OR%2018F-FLT%20AND%20rodentia)]

The use of [^18^F]FLT to monitor the response of tumors to antiproliferative treatment in mice was studied (11). The accumulation of [^18^F]FLT was significantly higher in blood, plasma, liver, kidneys, and small intestine and significantly lower in brain, spinal cord, heart, and muscle than [^18^F]FDG in C3H/Hej mice bearing the radiation-induced fibrosarcoma-1 tumor. The tumor-bearing mice were treated with 5-FU (165 mg/kg i.p.). Changes in tumor volume and biodistribution of [^18^F]FLT and [^18^F]FDG were measured in three groups of mice (n = 8-12/group): group a, untreated controls; group b, 24 h after 5-FU; and group c, 48 h after 5-FU. In addition, dynamic [^18^F]FLT PET imaging was performed on a small animal scanner for 60 min. Tumor [^18^F]FLT uptake decreased after 5-FU treatment. The drug-induced reduction in tumor [^18^F]FLT uptake was significantly greater than that of [^18^F]FDG. The PET image data confirmed smaller tumor [^18^F]FLT retention in group c compared with group a, despite a trend toward higher tracer delivery for group c. Other than phosphorylation in tumors, [^18^F]FLT was found to be metabolically stable in vivo. The decrease in tumor [^18^F]FLT uptake correlated with tumor proliferation and tumor volume changes after 5-FU treatment. Compared with group a, TK-1 levels were lower in group b (78.2%) but higher in group c (141.3%; P < 0.001). In contrast, a stepwise decrease in ATP levels was observed from group a to group b to group c (P < 0.001). In this murine model system, the radiotracer uptake was correlated with tumor proliferation. The decrease in [^18^F]FLT uptake after 5-FU treatment was more drastic than that of [^18^F]FDG. [^18^F]FLT is a marker for monitoring antiproliferative drug activity in oncology.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F-FLT%5BText%20Word%5D%20OR%20fluorothymidine%5BAll%20Fields%5D%29%20and%20%28dog%20or%20rabbit%20or%20pig%20or%20sheep%29)]

[^18^F]FLT was infused into normal dogs, as well as one dog with spontaneous lymphoma, and one with sarcoma before treatment (5). Dynamic PET imaging was performed for 60 min over the upper abdomen in normal dogs or over the tumors. For comparison, dynamic imaging with [^11^C]thymidine was also performed in two dogs. Images from normal dogs demonstrated a selective uptake in the marrow. There was also a high retention of FLT in the nose of the dog and the submandibular lymph node. The kidneys and the bladder showed a high uptake activity. The brain had a low uptake of FLT. The mean standardized uptake value (SUV) for FLT in dog marrow was 4.6 (4.1-5.5; n = 3), compared with 2.5 for [^11^C]thymidine (2.4-2.6; n = 2) There was a progressive FLT uptake in the bone marrow during the 60 min of imaging. On the other hand, [^11^C]thymidine, which is largely degraded within minutes of injection, did not accumulate in tissues after its initial uptake and retention in DNA. HPLC analysis of the dog urine after [^18^F]FLT administration showed that over 95% of the activity was present as unchanged [^18^F]FLT. Similarly, analysis of late blood samples (50 min) demonstrated that 90–97% of the activity remained as the parent compound. FLT was retained in cells as the phosphorylated form, and most FLT was intact when it was cleared by the kidneys. In a dog with spontaneous non-Hodgkin’s lymphoma, there was a greater uptake in the tumor (SUV, 7.1) than was seen for the marrow (SUV, 5.5). Also, in a dog with a large soft tissue sarcoma (11 cm in diameter), a rim of increased FLT accumulation (SUV, 3.1) was observed. The central region of the tumor showed little FLT uptake because it was necrotic.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F-FLT%5BText%20Word%5D%20AND%20primates%20NOT%20humans)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F-FLT%5BText%20Word%5D%20OR%20fluorothymidine%5BAll%20Fields%5D%29%20human)]

Dosimetry of [^18^F]FLT was calculated from the biodistribution data of 18 patients (12). The effective dose equivalent was estimated to be 0.031 mSv/MBq (114 mrem/mCi). The major radioactivity was in the bladder, liver, kidneys, and bone marrow. In 11 patients with non-small cell lung cancer, there was a strong correlation of [^18^F]FLT PET with cytochemical staining of nuclei with MIB-1 monoclonal antibody (13). In another study (14), 26 patients with pulmonary nodules on chest CT were examined with the uptake of [^18^F]FDG and [^18^F]FLT. Of 18 malignant tumors, 17 showed increased [^18^F]FDG PET uptake. [^18^F]FLT PET was falsely negative in the carcinoma, in another non-small cell lung cancer with a low proliferation index, and in a patient with lung metastases from colorectal cancer. Increased [^18^F]FLT uptake was related exclusively to malignant tumors. By contrast, [^18^F]FDG PET was falsely positive in 4 of 8 patients with benign lesions. Comparative studies of FLT and FDG were performed in patients with B-cell lymphoma (15), metastatic melanoma (16), breast cancer (17), and thoracic sarcoma (18).

## References

1 Kubota R., Yamada S., Kubota K., Ishiwata K., Tamahashi N., Ido T. (1992). Intratumoral distribution of fluorine-18-fluorodeoxyglucose in vivo: high accumulation in macrophages and granulation tissues studied by microautoradiography. J Nucl Med.
2 van Waarde A., Cobben D.C., Suurmeijer A.J., Maas B., Vaalburg W., de Vries E.F., Jager P.L., Hoekstra H.J., Elsinga P.H. (2004). Selectivity of 18F-FLT and 18F-FDG for differentiating tumor from inflammation in a rodent model. J Nucl Med.
3 Ishiwata K., Ido T., Abe Y., Matsuzawa T., Murakami M. (1985). Studies on 18F-labeled pyrimidines III. Biochemical investigation of 18F-labeled pyrimidines and comparison with 3H-deoxythymidine in tumor-bearing rats and mice. Eur J Nucl Med.
4 Sherley J.L., Kelly T.J. (1988). Regulation of human thymidine kinase during the cell cycle. J Biol Chem.
5 Shields A.F., Grierson J.R., Dohmen B.M., Machulla H.J., Stayanoff J.C., Lawhorn-Crews J.M., Obradovich J.E., Muzik O., Mangner T.J. (1998). Imaging proliferation in vivo with [F-18]FLT and positron emission tomography. Nat Med.
6 Grierson J.R., Shields A.F. (2000). Radiosynthesis of 3'-deoxy-3'-[(18)F]fluorothymidine: [(18)F]FLT for imaging of cellular proliferation in vivo. Nucl Med Biol.
7 Oh S.J., Mosdzianowski C., Chi D.Y., Kim J.Y., Kang S.H., Ryu J.S., Yeo J.S., Moon D.H. (2004). Fully automated synthesis system of 3'-deoxy-3'-[18F]fluorothymidine. Nucl Med Biol.
8 Seitz U., Wagner M., Neumaier B., Wawra E., Glatting G., Leder G., Schmid R.M., Reske S.N. (2002). Evaluation of pyrimidine metabolising enzymes and in vitro uptake of 3'-[(18)F]fluoro-3'-deoxythymidine ([(18)F]FLT) in pancreatic cancer cell lines. Eur J Nucl Med Mol Imaging.
9 Grierson J.R., Schwartz J.L., Muzi M., Jordan R., Krohn K.A. (2004). Metabolism of 3'-deoxy-3'-[F-18]fluorothymidine in proliferating A549 cells: validations for positron emission tomography. Nucl Med Biol.
10 Dittmann H., Dohmen B.M., Kehlbach R., Bartusek G., Pritzkow M., Sarbia M., Bares R. (2002). Early changes in [18F]FLT uptake after chemotherapy: an experimental study. Eur J Nucl Med Mol Imaging.
11 Barthel H., Cleij M.C., Collingridge D.R., Hutchinson O.C., Osman S., He Q., Luthra S.K., Brady F., Price P.M., Aboagye E.O. (2003). 3'-deoxy-3'-[18F]fluorothymidine as a new marker for monitoring tumor response to antiproliferative therapy in vivo with positron emission tomography. Cancer Res.
12 Vesselle H., Grierson J., Peterson L.M., Muzi M., Mankoff D.A., Krohn K.A. (2003). 18F-Fluorothymidine radiation dosimetry in human PET imaging studies. J Nucl Med.
13 Vesselle H., Grierson J., Muzi M., Pugsley J.M., Schmidt R.A., Rabinowitz P., Peterson L.M., Vallieres E., Wood D.E. (2002). In vivo validation of 3'deoxy-3'-[(18)F]fluorothymidine ([(18)F]FLT) as a proliferation imaging tracer in humans: correlation of [(18)F]FLT uptake by positron emission tomography with Ki-67 immunohistochemistry and flow cytometry in human lung tumors. Clin Cancer Res.
14 Buck A.K., Halter G., Schirrmeister H., Kotzerke J., Wurziger I., Glatting G., Mattfeldt T., Neumaier B., Reske S.N., Hetzel M. (2003). Imaging proliferation in lung tumors with PET: 18F-FLT versus 18F-FDG. J Nucl Med.
15 Wagner M., Seitz U., Buck A., Neumaier B., Schultheiss S., Bangerter M., Bommer M., Leithauser F., Wawra E., Munzert G., Reske S.N. (2003). 3'-[18F]fluoro-3'-deoxythymidine ([18F]-FLT) as positron emission tomography tracer for imaging proliferation in a murine B-Cell lymphoma model and in the human disease. Cancer Res.
16 Cobben D.C., Jager P.L., Elsinga P.H., Maas B., Suurmeijer A.J., Hoekstra H.J. (2003). 3'-18F-fluoro-3'-deoxy-L-thymidine: a new tracer for staging metastatic melanoma?. J Nucl Med.
17 Smyczek-Gargya B., Fersis N., Dittmann H., Vogel U., Reischl G., Machulla H.J., Wallwiener D., Bares R., Dohmen B.M. (2004). PET with [18F]fluorothymidine for imaging of primary breast cancer: a pilot study. Eur J Nucl Med Mol Imaging.
18 Dittmann H., Dohmen B.M., Paulsen F., Eichhorn K., Eschmann S.M., Horger M., Wehrmann M., Machulla H.J., Bares R. (2003). [18F]FLT PET for diagnosis and staging of thoracic tumours. Eur J Nucl Med Mol Imaging.